# Carbobenzoxy-capped Phe-Lys(Cy5)-acyloxymethyl ketone

Chemical name: | Carbobenzoxy-capped Phe-Lys(Cy5)-acyloxymethyl ketone
Abbreviated name: | GB123
Synonym: | Activity-based probe (ABP)
Agent Category: | Compounds
Target: | Cysteine cathepsin
Target Category: | Enzyme
Method of detection: | Optical imaging
Source of signal / contrast: | Cy5
Activation: | No
Studies: | - In vitro; - Rodents | Click on the PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=cathepsin) for additional information of the relevant substances.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=cysteine+cathepsins)]

The human cysteine cathepsins have 11 members (cathepsins B, C, H, F, K, L, O, S, V, W, and X/Z) and share a conserved active site that is formed by cysteine, histidine, and asparagine residues (1-5). Cathepsins B, L, H, F, O, X/Z, and C are expressed ubiquitously, whereas the expression of cathepsins S, K, W, and V are relatively organ-limited. Cysteine cathepsins interact with other proteases (aspartic, metallo, serine, and threonine) in a cascade-like manner, involving various physiological processes, including protein degradation, precursor protein activation, MHC-II–mediated antigen presentation, bone remodeling, keratinocytes differentiation, hair follicle cycle, reproduction, and apoptosis (6, 7). Increased expression and activity, and relocalization to the plasma membrane of cysteine cathepsins are associated with the pathogenesis of a number of human diseases such as cancer, atherosclerosis, and neurodegenerative diseases, and changes related to cysteine cathepsins have been shown to be of diagnostic and prognostic value for the diseases (2, 8-11).

Significant efforts have been made in developing optical molecular probes of protease activity (4, 7, 12, 13). These probes are either substrate-based or activity-based, providing a readout of the enzyme activity rather than simple protein abundance. Substrate-based probes (SBPs) are designed using fluorescent peptide sequences tethered to a large polymer or dendramer backbone, and these SBPs are internally quenched by the high density of fluorophores loaded onto the backbone structure. Similar to conventional enzymatic tests, SBPs appear to be less reliable because of overlapping substrate specificities, enzymatic activity instability, and interactions with endogenous inhibitors. Activity-based probes (ABPs) label target proteases through the formation of a covalent bond with the active site cysteine. The selectivity of an ABP is controlled by both its peptide selectivity sequence and reactive functional group. The fluorescent reporter allows probe-labeled cathepsins to be directly visualized. Because ABPs tend to be small molecules, the in vivo half-lives of ABPs are relatively short, which results in the production of high-contrast images. A drawback of using a covalent probe is the lack of signal amplification because the target proteases are inactivated upon binding the probe. However, sufficient levels of the active proteases have been found to exist in tumor tissues, which allows the generation of reasonable contrast images using noninvasive methods (4, 7, 12).

Blum et al. synthesized a group of near-infrared fluorescent activity-based probes (NIRF-ABPs) for noninvasive optical imaging of cysteine protease activity (4, 7, 12, 14). These probes can be subgrouped into quenched ABPs (qABPs) (e.g., GB117, GB119, GB135, and GB137) and nonquenched ABPs (e.g., GB111, GB123, and GB138). In short, the probes consist of a reactive group of peptide acyloxymethyl ketone (AOMK) that targets diverse members of cysteine cathepsins. The ketone in AOMK reacts with the cysteine in the enzyme active site and produces a stable thiomethyl ketone adduct. The covalent binding involves the loss of the acyloxy group of AOMK. Thus, a probe carrying a fluorescent reporter group on its peptide scaffold and a highly efficient quenching molecule attached to the acyloxy-losing group should result in a quenched probe that only becomes fluorescent upon covalent binding with an enzyme. In addition, a spacer is designed to reduce the steric congestion between the reporter and the fluorescence quencher. Blum et al. have shown that the NIRF-ABPs are nontoxic to cells, reasonably water soluble, potentially valuable as imaging agents for disease diagnosis, and powerful tools for in vivo preclinical and clinical testing of small-molecule therapeutic agents. Although NIRF-ABPs present different features regarding stability, specificity, and kinetics, the quenched probes can be used to image specific protease activity at considerably earlier time points than can be used for substrate-based methods or nonquenched ABPs. However, high levels of signal in large organs with high cathepsin activity such as liver, kidney, and spleen make activity-based imaging of specific locations within the central body cavity difficult. In this chapter, the synthesis and analytic results of nonquenched ABP GB123 were introduced. GB123 is the Cy5 version of the first generation of nonquenched ABP GB111.

### Related Resource Links:

1) Cysteine cathepsin imaging-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html):

- Substrate-based probes: Cy5.5-PL-MPEG (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=PL-MPEG-Cy55), Cy5.5-GHPGGPQK(Fitc)C-PL-MPEG (Cy5.5-CatK-PGC) (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=CatK-PL-MPEG-Cy55),
- Activity-based probes: GB137 (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=GB137)

2) Gene and protein information of human cathepsins (http://www.ncbi.nlm.nih.gov/protein/?term=cathepsin+and+human)

3) Cathepsin-related resource in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=cathepsin)

4) Cathepsin-related substances in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=cathepsin)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Blum+G)]

GB123 is the Cy5 version of the first-generation nonquenched ABP GB111, which has been introduced in another chapter of MICAD (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html) (4, 12, 14). Briefly, the fully protected carbobenzoxy-capped Phe-Lys dipeptide was synthesized (85% purity and 99% yield relative to resin loading) and then converted to bromo-methyl ketone (BMK, 91% yield). AOMK was obtained by converting the BMK via N-trityl–protected glycine (25% yield). The final product GB123 was generated by coupling Cy5 fluorophore on the side chain of lysine after removal of the t-butoxy carbonyl protecting group (48% yield). GB125 (Cy5-N-benzyloxycarbonyl-Phe-Lys) was also generated as a control probe in a similar manner; however, GB125 lacked the AOMK reactive group and the Cy5 was coupled to the N-ε-free amine (69.3% yield). The molecular weights were 1,256.5 and 1,109.4 for GB123 and GB125, respectively (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Blum+G)]

Blum et al. tested the probes for their sensitivity to serum exposure by preincubating the probes for either 1 h or 4 h before adding them to the monolayer of NIH-3T3 cells to label target proteases (4). Cell labeling showed that GB123 was insensitive to serum even after preincubation for 4 h, but GB119 (the quenched version of the GB123 probe) completely lost its ability to label the target proteases even after preincubation for 1 h. The increased serum sensitivity of GB119 has been confirmed to be caused by the presence of a glycine spacer adjacent to the reactive carbon methylene group of the AOMK.

To verify the cell permeability and labeling specificity of GB123, intact C2C12/Hras1 cells were preincubated with either JPM-OEt, a general papain-family inhibitor, or vehicle control before cell labeling with GB123 or GB125. The specific probe GB123 showed punctate labeling of lysosomal compartments that was overlapped with the acidotropic lysosomal marker LysoTracker. Pretreatment with JPM-OEt completely blocked GB123 staining, which suggested that the signal was due to a specific modification of cysteine cathepsins. On the contrary, while the control probe GB125 accumulated in cells without washout (data not shown), after washout there was no labeling with GB125, which confirmed that the lack of labeling was not caused by a loss of cell permeability. These data indicate that both probes freely penetrated cells, but only GB123 was retained as a result of the irreversible modification of lysosomal cysteine cathepsins (4).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=Blum+G)]

To decide on an optimal cell line for use in tumor imaging studies, Blum et al. profiled the cysteine cathepsin activities in a number of commonly used cancer cell lines (4). In all cell lines tested, specific labeled proteases in the 20–30 kDa size range were detected with SDS-PAGE gel analysis. The highest cathepsin activity was observed in the mouse skeletal myoblast cell line (C2C12) retrovirally transduced with the Hras1 oncogene (C2C12/Hras1). A similar labeling pattern, although with reduced intensity, was observed in the human breast cancer cell lines MDA-MB-231, MDA-MB-435, and MDA-MB-231 MFP. These lines were selected for imaging studies because they express similar cathepsins but show marked differences in overall activity.

Imaging studies were performed in BALB/c nude mice bearing subcutaneous MDA-MB-231, MDA-MB-435, or C2C12/Hras1 tumor grafts (n = 2–4 mice/group) (4). After tail vein injection of GB123, the fluorescent probe rapidly circulated throughout the animal, and high fluorescent signals were seen in virtually all tissues, including the tumors. Thereafter, the investigators observed that the signal faded continuously over most regions of the body but remained elevated in the tumors. The control probe GB125, on the other hand, was rapidly cleared and no fluorescent signal above background was observed by the 5-h time point. After imaging, tissues were collected for biochemical analysis. With SDS-PAGE gel analysis, three predominant labeled proteins were observed in the 20–30 kDa size range, which were similar to the labeled cathepsins observed in the parent cell lines. The 30- and 23-kDa proteins were confirmed to be the cathepsin B and the heavy chain form of cathepsin L, respectively. Although Blum et al. cannot determine the identity of the 25-kDa protein with available antibodies, they consider it to be a cysteine cathepsin given that its labeling can be blocked by treatment of animals with specific inhibitors. The overall labeling intensity of the cathepsins observed with gel analysis strongly correlated with the intensity of the signal observed in the whole-body images. These results suggest that the signal observed in tumors and other tissues results from specific probe modification of active cysteine cathepsins.

To further confirm that the signals observed in whole-body images were due to protease activity, Blum et al. pretreated the animals with intraperitoneal injection of JPM-OEt to reduce protease activity before imaging (4). However, all of the attempts to reduce cysteine cathepsin activity in tumors failed in both imaging and SDS-PAGE analysis of the tissue extracts. Lack of inhibition is explained by the nature of grafted tumors, which may generally be less accessible to this class of small-molecule inhibitors than tumors that develop in situ in their native microenvironment. Therefore, the investigators switched to the MDA-MB-231 MFP cells and a broad-spectrum inhibitor K11777, which has more favorable cell permeability properties. In addition, the mice were pretreated for 5 days before imaging. Imaging showed that the specific signal in tumors at the 10-h time point was reduced by 60–80% in mice treated with K11777 relative to control mice. SDS-PAGE analysis of the tissue extracts also showed reduced signal intensity by 50–80% in the K11777-treated mice. Labeling profiles in all tissues from both treated mice and control mice demonstrated the same pattern of active cathepsins that was observed previously.

These data support the notion that NIRF-ABPs provide a fluorescent readout of protease activity in a living animal and that the modulation of this activity using small-molecule therapeutics can be monitored with direct, whole-body imaging methods (4, 7, 12, 14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Colbert J.D., Matthews S.P., Miller G., Watts C. (2009). Diverse regulatory roles for lysosomal proteases in the immune response. Eur J Immunol.
2 Affara N.I., Andreu P., Coussens L.M. (2009). Delineating protease functions during cancer development. Methods Mol Biol.
3 Cox J.L. (2009). Cystatins and cancer. Front Biosci.
4 Blum G., von Degenfeld G., Merchant M.J., Blau H.M., Bogyo M. (2007). Noninvasive optical imaging of cysteine protease activity using fluorescently quenched activity-based probes. Nat Chem Biol.
5 Hang H.C., Loureiro J., Spooner E., van der Velden A.W., Kim Y.M., Pollington A.M., Maehr R., Starnbach M.N., Ploegh H.L. (2006). Mechanism-based probe for the analysis of cathepsin cysteine proteases in living cells. ACS Chem Biol.
6 Palermo C., Joyce J.A. (2008). Cysteine cathepsin proteases as pharmacological targets in cancer. Trends Pharmacol Sci.
7 Blum G. (2008). Use of fluorescent imaging to investigate pathological protease activity. Curr Opin Drug Discov Devel.
8 Cavallo-Medved D., Rudy D., Blum G., Bogyo M., Caglic D., Sloane B.F. (2009). Live-cell imaging demonstrates extracellular matrix degradation in association with active cathepsin B in caveolae of endothelial cells during tube formation. Exp Cell Res.
9 Gounaris E., Tung C.H., Restaino C., Maehr R., Kohler R., Joyce J.A., Ploegh H.L., Barrett T.A., Weissleder R., Khazaie K. (2008). Live imaging of cysteine-cathepsin activity reveals dynamics of focal inflammation, angiogenesis, and polyp growth. PLoS One.
10 Lutgens S.P., Cleutjens K.B., Daemen M.J., Heeneman S. (2007). Cathepsin cysteine proteases in cardiovascular disease. FASEB J.
11 Joyce J.A., Baruch A., Chehade K., Meyer-Morse N., Giraudo E., Tsai F.Y., Greenbaum D.C., Hager J.H., Bogyo M., Hanahan D. (2004). Cathepsin cysteine proteases are effectors of invasive growth and angiogenesis during multistage tumorigenesis. Cancer Cell.
12 Blum G., Mullins S.R., Keren K., Fonovic M., Jedeszko C., Rice M.J., Sloane B.F., Bogyo M. (2005). Dynamic imaging of protease activity with fluorescently quenched activity-based probes. Nat Chem Biol.
13 Yang Z., Fonovic M., Verhelst S.H., Blum G., Bogyo M. (2009). Evaluation of alpha,beta-unsaturated ketone-based probes for papain-family cysteine proteases. Bioorg Med Chem.
14 Blum G., Weimer R.M., Edgington L.E., Adams W., Bogyo M. (2009). Comparative assessment of substrates and activity based probes as tools for non-invasive optical imaging of cysteine protease activity. PLoS One.